# Poly(ethylene glycol)-coated gold nanocages bioconjugated with [Nle^4^,D-Phe^7^]-α-melanotropin-stimulating hormone

Chemical name: | Poly(ethylene glycol)-coated gold nanocages bioconjugated with [Nle^4^,D-Phe^7^]-α-melanotropin-stimulating hormone
Abbreviated name: | [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 receptor, MC1R
Target category: | Receptor
Method of detection: | Ultrasound, photoacoustic tomography (PAT) imaging
Source of signal: | Gold (Au)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gold%20nanocages)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Photoacoustic imaging (PAI) is an emerging hybrid biomedical imaging modality based on the photoacoustic effect. In PAI, non-ionizing optical pulses are delivered into biological tissues. Some of the delivered energy is absorbed and converted into heat, leading to transient thermoelastic expansion and thus ultrasonic emission. The generated ultrasonic waves are then detected by ultrasonic transducers to form images. It is known that optical absorption is closely associated with physiological properties, such as hemoglobin concentration and oxygen saturation. As a result, the magnitude of the ultrasonic emission (i.e., photoacoustic signal), which is proportional to the local energy deposition, reveals physiologically specific optical absorption contrast and tissue structures. However, exogenous NIR contrast agents are necessary to overcome the intrinsic low tissue- and hemoglobin- absorption and scattering of tissue. On the other hand, these small molecules exhibit fast clearance, small optical absorption cross section, and non-targeted specificity. Therefore, there is a need for contrast agents with long blood circulation and targeted specificity.

Gold (Au) nanoparticles have been studied as molecular imaging agents because of their bright NIR fluorescence emission of 700–900 nm and low toxicity (6, 7). They can be tuned to emit in a range of wavelengths by changing their sizes, shapes, and composition, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies. Au nanoparticles have been approved by the United States Food and Drug Administration for the treatment of patients with rheumatoid arthritis. Au nanoparticles have been studied as contrast agents in X-ray/computed tomography, NIR optical coherence tomography, PAI, and photoacoustic tomography (PAT) (8). NIR Au nanocages (AuNCs) are biocompatible, have low toxicity, and are tunable to strong NIR absorption (9). They have an outer edge of ~50 nm and an inner edge of ~42 nm, with a wall thickness of ~4 nm. Yang et al. (10) have performed PAT of the cerebral cortex of rats with poly(ethylene glycol)-coated AuNCs (PEG-AuNCs) as an optical contrast agent. The investigators observed an enhanced optical contrast in the vasculature in the cerebral cortex. Song et al. (11) demonstrated the use of Au nanocages as a PAI probe for detection of sentinel lymph nodes in rats.

Malignant melanoma is the deadliest form of skin cancer (12). Early and accurate diagnosis is necessary for surgery and successful treatment (13). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (14). Most cutaneous cell types express MC receptors, proopiomelanocortin (POMC), and prohormone convertases, and they also release MCs. However, these receptors have been found to be overexpressed in melanoma cells. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (15) in the regulation of skin pigmentation via MC1R. Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R, which is overexpressed on human and mouse melanoma cells (16-20). Kim et al. (21) have evaluated [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs for in vivo PAT imaging of melanomas in mice.

### Related Resource Links:

- Chapters in MICAD (MC1R (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=MSH+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), Gold imaging (http://www.ncbi.nlm.nih.gov/books?term=Gold%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (MC1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157))
- Articles in OMIM (MC1R (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=155555))
- Clinical trials (MC1R (http://www.clinicaltrials.gov/ct2/results?term=MC1R), Gold nanoparticles (http://www.clinicaltrials.gov/ct2/results?term=gold+AND+nanoparticles))
- Drug information in FDA (Gold nanoparticles (http://google2.fda.gov/search?q=gold%2BAND%2Brheumatoid%2Barthritis&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MSH%20AuNCs%20and%20synthesis)]

Kim et al. (21) reported the synthesis of PEG-AuNCs by incubation of HAuCl_4_ (0.5 mM) and Ag nanocubes containing poly(vinyl pyrrolidone) (PVP, 0.1 mg/ml) with stirring for 10 min at 100°C. Upon cooling to room temperature, excess NaCl was added to remove Ag as AgCl. The supernatant was discarded and the AuNCs were resuspended in water. The AuNC alloy was composed of 70% Au and 30% Ag. AuNCs were washed six times to remove PVP and NaCl. AuNC surfaces were functionalized with PEG by adding 1 mL of a 1-mM succinimidyl propionyl PEG-SH (5 kDa) to AuNCs. The suspension was incubated for 8 h at room temperature. Residual succinimidyl propionyl PEG-SH was removed by centrifugation. [Nle^4^,D-Phe^7^]-α-MSH was then incubated with a suspension of the AuNCs for 12 h at 7°C. [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs were isolated with centrifugation. AuNCs have an outer edge of ~46 nm and a wall thickness of ~7 nm as estimated with transmission electron microscopy. The number of [Nle^4^,D-Phe^7^]-α-MSH moieties per AuNC was not reported. [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs and PEG-AuNcs had maximum optical absorption at ~800 nm with a detection limit of 4.5 pM (Au) with PAI.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MSH%20AuNCs%20and%20in%20vitro)]

B16-F0 mouse melanoma cells accumulated 123 ± 11 and 633 ± 121 [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs/cell (measured with inductively coupled plasma mass spectrometry (ICP-MS)) after 6 h and 24 h of incubation with 0.01 nM AuNCs (21), respectively. On the other hand, B16-F0 mouse melanoma cells accumulated 35 ± 30 and 182 ± 10 PEG-AuNCs/cell after 6 h and 24 h of incubation, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MSH%20AuNCs%20and%20rodentia)]

Kim et al. (21) performed noninvasive PAT of mice (n = 4) bearing B16-F0 melanoma after intravenous injection of a single dose (1 nmol) of [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs or PEG-AuNcs. PAT scanning began immediately after injection and continued for ~6 h with the laser wavelength at 778 nm and ultrasound frequency of 10 MHz. PAT images revealed a greater optical contrast in the tumor after [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs injection compared with before injection. There was a gradual enhancement of the PA signal in the tumor with a maximum value of 38 ± 6% at 6 h after injection. In mice injected with PEG-AuNCs, there was a maximum enhancement of 13 ± 2% at 6 h after injection. Therefore, tumor accumulation of [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs was significantly higher than that of PEG-AuNCs (P = 0.007). Ex vivo ICP-MS analysis showed that the average number of [Nle^4^,D-Phe^7^]-α-MSH-PEG-AuNCs per tumor mass was 3.6 ± 1.0 × 10^8^ AuNCs/g, whereas with PEG-AuNCs there were only 1.0 ± 1.0 × 10^8^ AuNCs/g (P = 0.02). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MSH%20AuNCs%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MSH%20AuNCs%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MSH%20AuNCs%20and%20human)]

No publication is currently available.

## NIH Support

R01 EB008085, R01 EB000712, U54 CA136398, 5DP1 OD000798-04

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Vosch T., Antoku Y., Hsiang J.C., Richards C.I., Gonzalez J.I., Dickson R.M. (2007). Strongly emissive individual DNA-encapsulated Ag nanoclusters as single-molecule fluorophores. Proc Natl Acad Sci U S A.
7 Chithrani B.D., Ghazani A.A., Chan W.C. (2006). Determining the size and shape dependence of gold nanoparticle uptake into mammalian cells. Nano Lett.
8 Choi H.S., Frangioni J.V. (2010). Nanoparticles for biomedical imaging: fundamentals of clinical translation. Mol Imaging.
9 Yang X., Stein E.W., Ashkenazi S., Wang L.V. (2009). Nanoparticles for photoacoustic imaging. Wiley Interdiscip Rev Nanomed Nanobiotechnol.
10 Yang X., Skrabalak S.E., Li Z.Y., Xia Y., Wang L.V. (2007). Photoacoustic tomography of a rat cerebral cortex in vivo with au nanocages as an optical contrast agent. Nano Lett.
11 Song K.H., Kim C., Cobley C.M., Xia Y., Wang L.V. (2009). Near-infrared gold nanocages as a new class of tracers for photoacoustic sentinel lymph node mapping on a rat model. Nano Lett.
12 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
13 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
14 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
15 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
16 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
17 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
18 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
19 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
20 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
21 Kim C., Cho E.C., Chen J., Song K.H., Au L., Favazza C., Zhang Q., Cobley C.M., Gao F., Xia Y., Wang L.V. (2010). In vivo molecular photoacoustic tomography of melanomas targeted by bioconjugated gold nanocages. ACS Nano.